# ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid- Affibody Z_HER2:342-pep2_

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Affibody Z_HER2:342-pep2_
Abbreviated name: | ^111^In-DOTA-Z_HER2:342-pep2_
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | EGF HER2 receptor
Target category: | Receptor
Method of detection: | SPECT, gamma planar
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342)]

Epidermal growth factor (EGF) is a cytokine that comprises 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab -F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed based on the 58-amino-acid Z-domain residues from one of the IgG-binding domains of staphylococcal protein A (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values of <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. A synthetic Affibody molecule was successfully produced as DOTA-Z_HER2:342-pep2_ for labeling with ^111^In. ^111^In-DOTA-Z_HER2:342-pep2_ has been evaluated in nude mice bearing human SKOV-3 ovarian cancer cells (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20synthesis)]

DOTA-Z_HER2:342-pep2_ was prepared by standard peptide synthesis (18). DOTA-Z_HER2:342-pep2_ in 0.2 M ammonium acetate buffer (pH 5.25) was mixed with a predetermined amount of ^111^InCl_3_. The mixture was incubated for 30 or 60 min at different temperatures (room temperature, 37°C, 50°C, and 90°C). Under all conditions tested, the labeling efficiency of ^111^In incorporation was 96% and 98% after incubation for 30 or 60 min at room temperature, respectively; 98% for both times at 37°C; 99% for both times at 50°C; and 99% for 30 min at 90°C. Specific activities of the preparations were not mentioned.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20in%20vitro)]

Orlova et al. (18) performed binding experiments with DOTA-Z_HER2:342-pep2_ with use of a Biacore sensor chip immobilized with extracellular domain of HER2 (HER2_ECD_) or chimeric HER2/Fc fusion protein. The K_d_ values of DOTA-Z_HER2:342-pep2_ were calculated to be 65 pM for HER2_ECD_ and 78 pM for chimeric HER2/Fc fusion protein. The K_d_ values of His_6_-Z_HER2:342_ were 20 pM for HER2_ECD_ and 29 pM for chimeric HER2/Fc fusion protein. Hence, the binding affinity of the synthetic Affibody molecule DOTA-Z_HER2:342-pep2_ was approximately two-fold lower than the recombinant Affibody molecule His_6_-Z_HER2:342_.

In vitro binding specificity tests showed that binding of ^111^In-DOTA-Z_HER2:342-pep2_ to SKOV-3 cells expressing HER2 was receptor-mediated because saturation of receptors by preincubation with non-labeled His_6_-Z_HER2:342_ significantly decreased binding of ^111^In-DOTA-Z_HER2:342-pep2_ (P < 0.0001). The antigen binding capacity of ^111^In-DOTA-Z_HER2:342-pep2_ was 82–86%. After an initial reduction, the cell-bound radioactivity remained constant at ~90% of the initially bound activity for up to 24 h when the cells were incubated with ^111^In-DOTA-Z_HER2:342-pep2_. In contrast, cells incubated with ^125^I-His_6_-Z_HER2:342_ lost ~40% of the original cell-associated radioactivity during the first 4 h and an additional 20% at 29 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20rodentia)]

Orlova et al. (18) monitored biodistribution using single-photon emission computed tomography (SPECT) analysis after injection of therapeutic doses of 0.1 MBq (2.7 μCi) ^111^In-DOTA-Z_HER2:342-pep2_ in nude mice bearing tumor xenografts. Tumor radioactivity was measured 4 h after tracer injection. The tumor xenograft with the highest uptake was the human breast cancer cell line BT474 (39.9% injected dose per gram (ID/g)), followed by the human ovarian cancer cell line SKOV-3 (13.3% ID/g), the human breast cancer cell line MCF7 (12.4% ID/g), the human breast cancer cell line MDA-MB-231 (4.4% ID/g), and the human Ramos B lymphoma cell line with no HER2 expression (0.1% ID/g). The uptake values in these tumors were proportional to their HER2 expression levels. Pretreatment with Z_HER2:342_ significantly inhibited the ^111^In-DOTA-Z_HER2:342-pep2_ uptake values in all HER2-expressing tumors. The kidney was the only organ that had a higher accumulation than the tumors (256% ID/g at 4 h). The tumor/blood ratio was 8 ± 1 at 1 h and 121 ± 33 at 72 h. SPECT gamma imaging revealed that the SKOV-3 tumors were clearly visualized in mice injected with ^111^In-DOTA-Z_HER2:342-pep2_. In mice pretreated with Z_HER2:342_, the tumors could not be visualized with ^111^In-DOTA-Z_HER2:342-pep2_. Furthermore, the tumors could not be visualized by injection of a control-labeled nonspecific peptide (^111^In-DOTA-Z_taq4:5_).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Orlova A., Tolmachev V., Pehrson R., Lindborg M., Tran T., Sandstrom M., Nilsson F.Y., Wennborg A., Abrahmsen L., Feldwisch J. (2007). Synthetic affibody molecules: a novel class of affinity ligands for molecular imaging of HER2-expressing malignant tumors. Cancer Res.